# Cyclo(Cys-Arg-Gly-Asp-Cys)-Gly-Lys-Cy5.5

Chemical name: | Cyclo(Cys-Arg-Gly-Asp-Cys)-Gly-Lys-Cy5.5
Abbreviated name: | c(CRGDC)-GK-Cy5.5
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD%5BAll%20Fields%5D%20AND%20%22CY5.5%20cyanine%20dye%22%5BSubstance%20Name%5D)]

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive alternative to radionuclide imaging in small animals or with probes in close proximity of the target in humans (4, 5). Among the various optical imaging agents, only indocyanine green (ICG (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=15096)), with NIR fluorescence absorption at 780 nm and emission at 820 nm, is approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment. It is also under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications, such as optical imaging and mapping of both the lymphatic vessels and lymph nodes in cancer patients for surgical dissection of tumors and endoscopic imaging of the pancreas and colon.

Integrins are a family of cell-surface heterodimeric glycoproteins that mediate diverse biological events involving cell–cell and cell–matrix interactions (6). They consist of an α and a β subunit, and they are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor class affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (7-12). The α_v_β_3_ integrin is strongly expressed on tumor cells and activated endothelial cells. In contrast, expression of α_v_β_3_ integrin is weak on resting endothelial cells and most normal tissues. The α_v_β_3_ antagonists are being studied as anti-tumor and anti-angiogenic agents (9, 13, 14), and the agonists are being studied as angiogenic agents for coronary angiogenesis (15, 16). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (17).

Cyclo(RGDyK) was conjugated with Cy5.5 to study in vivo biodistribution of the tracer in tumor-bearing mice. Cy5.5 is a NIR fluorescent dye with an absorbance maximum at 675 nm and an emission maximum at 694 nm, with a high extinction coefficient of 250,000 (mol/L)^–1^cm^–1^. c(RGDyK)-Cy5.5 was found to have high and long-lasting accumulation in α_v_β_3_-positve U87MG human glioblastoma tumor cells in nude mice (18). The binding of c(RGDyK)-Cy5.5 to the integrin receptor was found to be specific both in vitro and in vivo. von Wallbrunn et al. (19) performed optical NIR fluorescence imaging studies using a two-dimensional planar fluorescence reflectance imaging system and three-dimensional fluorescence-mediated tomography (FMT) of cyclo(Cys-Arg-Gly-Asp-Cys)-Gly-Lys-Cy5.5 (c(CRGDC)-GK-Cy5.5) in tumor-bearing nude mice.

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD%5BAll%20Fields%5D%20AND%20%22CY5.5%20cyanine%20dye%22%5BSubstance%20Name%5Dand%20synthesis)]

Cy5.5 monofunctional N-hydroxysuccinimide (NHS) ester was used to conjugate c(CRGDC)-GK to form c(CRGDC)-GK-Cy5.5, which was purified with high-performance liquid chromatography (19). Chemical yields of 75%–90% were obtained. The NHS ester of Cy5.5 was reacted with the ε-amino group of the lysine in c(CRGDC)-GK. The identity of c(CRGDC)-GK-Cy5.5 was confirmed with high-resolution electrospray mass spectrometry.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD%5BAll%20Fields%5D%20AND%20%22CY5.5%20cyanine%20dye%22%5BSubstance%20Name%5D%20AND%20%28%22in%20vitro%22%5BMeSH%20Terms%5D%20OR%20in%20vitro%5BText%20Word%5D%29)]

Flow cytometry analysis showed that ~98% of human melanoma M21 cells, ~16% of human adenocarcinoma MCF-7 cells, and ~1% of human fibrosarcoma HT-1008 cells were positive for the α_v_β_3_ receptors (19). Binding of c(CRGDC)-GK-Cy5.5 to the three cell types was analyzed with fluorescence microscopy. M21cells exhibited a higher fluorescence intensity signal than MCF-7 cells, whereas little intensity signal was observed in the HT-1008 cells. The binding of c(CRGDC)-GK-Cy5.5 to M21 cells could be blocked with ten-fold excess of c(CRGDC)-GK.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD%5BAll%20Fields%5D%20AND%20%22CY5.5%20cyanine%20dye%22%5BSubstance%20Name%5D%20AND%20rodentia)]

von Wallbrunn et al. (19) used FRI and FMT to perform biodistribution studies of c(CRGDC)-GK-Cy5.5 in nude mice (n = 5/group) bearing M21 tumors. Surface-weighted FRI studies were performed at 1, 3, and 24 h after injection of 2 nmol c(CRGDC)-GK-Cy5.5. The tumor accumulation of c(CRGDC)-GK-Cy5.5 could be clearly seen from 1 h to 24 h. The tumor/background ratios were 1.33 ± 0.14 and 1.46 ± 0.31 at 1 h and 24 h after injection. Pretreatment with 200 nmol c(CRGDC)-GK 10 min before injection of c(CRGDC)-GK-Cy5.5 reduced the tumor/background ratio to 1.13 ± 0.13 at 1 h after injection (P < 0.05).

FMT studies were performed at 1, 3, 5, and 24 h after injection of c(CRGDC)-GK-Cy5.5 in mice bearing M21 (n = 5), MCF-7 (n = 5), or HT-1008 (n = 6) tumors. Quantitative analysis of NIF optical images at 1 h after injection showed Cy5.5 concentrations of 417.6 ± 105.8 nM, 353.7 ± 54.0 nM, and 262.8 ± 155.4 nM in the M21, MCF-7, and HT-1008 tumors, respectively. A maximal accumulation was observed at 1 h in the tumors, which slowly washed out over time. A strong fluorescence signal was observed in the liver (269.1 ± 65.5 nM Cy5.5) at 1 h. The tumor/muscle ratios at 1 h were 6.4, 5.6, and 4.0 for M21, MCF-7, and HT-1008 tumors, respectively. The tracer accumulation could be blocked by 30% (P < 0.05) after pretreatment (10 min) with 100 nmol c(CRGDC)-GK in M21 tumors. Western blotting of M21, MCF-7, and HT-1080 cell and tumor tissue lysates using a murine β_3_-specific monoclonal antibody showed a similar expression of the murine β_3_ subunit on the tumor tissue but not on the human tumor cells. The higher binding of c(CRGDC)-GK-Cy5.5 on the M21 tumor tissue is probably due to binding of c(CRGDC)-GK-Cy5.5 to both the tumor vasculature and cells (expression of α_v_β_3_ on M21 cells is higher than that on MCF-7 and HT-1080 cells). This proves to be a noninvasive method for imaging tumors in mice by using these two optical imaging techniques. FMT imaging allows three-dimensional reconstruction of NIR fluorescence distribution, which can be quantified.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD%5BAll%20Fields%5D%20AND%20%22CY5.5%20cyanine%20dye%22%5BSubstance%5D%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD%5BAll%20Fields%5D%20AND%20%22CY5.5%20cyanine%20dye%22%5BSubstance%20Name%5D%20AND%20primates%20NOT%20humans)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD%5BAll%20Fields%5D%20AND%20%22CY5.5%20cyanine%20dye%22%5BSubstance%20Name%5D%20AND%20humans%20not%20cell%20line)]

No publication is currently available.

## Reference

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
3 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
4 Frangioni J.V. (2003). In vivo near-infrared fluorescence imaging. Curr Opin Chem Biol.
5 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
6 Hynes R.O. (2002). A reevaluation of integrins as regulators of angiogenesis. Nat Med.
7 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
8 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
9 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
10 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
11 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
12 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
13 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
14 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
15 Sadeghi M.M., Krassilnikova S., Zhang J., Gharaei A.A., Fassaei H.R., Esmailzadeh L., Kooshkabadi A., Edwards S., Yalamanchili P., Harris T.D., Sinusas A.J., Zaret B.L., Bender J.R. (2004). Detection of injury-induced vascular remodeling by targeting activated alphavbeta3 integrin in vivo. Circulation.
16 Sinusas A.J. (2004). Imaging of angiogenesis. J Nucl Cardiol.
17 Haubner R., Beer A.J., Wang H., Chen X. (2010). Positron emission tomography tracers for imaging angiogenesis. Eur J Nucl Med Mol Imaging.
18 Chen X., Conti P.S., Moats R.A. (2004). In vivo near-infrared fluorescence imaging of integrin alphavbeta3 in brain tumor xenografts. Cancer Res.
19 von Wallbrunn A., Holtke C., Zuhlsdorf M., Heindel W., Schafers M., Bremer C. (2007). In vivo imaging of integrin alpha v beta 3 expression using fluorescence-mediated tomography. Eur J Nucl Med Mol Imaging.